# Perfluoro-15-crown-5 ether-labeled dendritic cells

Chemical name: | Perfluoro-15-crown-5 ether-labeled dendritic cells
Abbreviated name: | PFPE-DCs
Synonym:
Agent category: | Labeled cell
Target: | Other
Target category: | Other –inflamed tissue
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | ^19^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PFPE + DCs)]

Dendritic cells (DCs), known as antigen-presenting cells, are found in almost all peripheral tissues and in primary/secondary lymphoid organs (1). DCs are the initiator and modulator in the adaptive immune responses against bacteria, viruses, allergens, and tumor antigens (2). DCs in peripheral tissues are responsible for the capture of antigens (3). In the absence of inflammation, DCs remain in an immature state. The captured antigens are transported with DCs to the lymph node, but no co-stimulatory activation to T cells occurs. In the presence of inflammation, numerous mature DCs migrate to the draining lymph nodes. During migration, the antigens are processed into small peptides bound to the major histocompatibility complex (MHC) on the surface of the DCs. At the lymph nodes, mature DCs present the MHC-peptide complex to naïve T cells (CD4^+^ T helper cells and cytolytic CD8^+^ T cells) to activate them. After activation, a series of immune responses are completed through the interactions of T cells with other cells and molecules such as B cells for antibody formation, macrophages for cytokine releases, and targets for lysis (1). Behaving as mobile sentinels, DCs bring antigens to T cells and express co-stimulators to induce immunity. DCs have been used in many clinical trials to treat cancers and immunological disorders (4). Because the migratory properties of DCs are directly related to their function (5), non-invasive tracking of DCs becomes very important to clinic applications (2).

Being the only stable isotope of fluorine, with a natural abundance of ~100%, ^19^F has a nuclear spin 1/2 with a large gyromagnetic ratio (γ ~40.05 MHz/T) (6). The small γ difference between the ^19^F and ^1^H (~6%) allows the use of existing proton nuclear magnetic resonance (NMR) instrumentation with minor adjustments to detect fluorinated species at high sensitivity (~83% relative to ^1^H). Endogenous fluorine in vivo is found primarily in bones and teeth as solid fluorides, which have very short T_2_ relaxation times and result in an undetectable signal with NMR imaging. Therefore, exogenously administered fluorinated tracers can be used to track various biological processes in vivo. For example, perfluorocarbons (PFCs) are used to measure oxygen tensions in tissues and tumors (7). The lack of background ^19^F signal is advantageous in in vivo applications, but additional ^1^H images are required to provide anatomic interpretations. PFCs are extremely hydrophobic and do not dissolve in blood directly; they normally are formulated as biocompatible emulsions for intravenous administration (6). Inside the body, the PFC particles are cleared from circulation by phagocytes/macrophages or by respiration within several hours or days, depending on the administered dose, particle size, and PFCs (8). Many commercial PFC emulsions have been found to be nontoxic or do not cause any health problems other than tissue swelling (6). Perfluoro-15-crown-5 ether (perfluoropolyether, PFPE), a commonly used PFC, contains 20 equivalent ^19^F spins that generate a single resonance (-92.5 ppm) in NMR imaging (9). This singlet simplifies its images such that no chemical shift–induced artifact is expected. PFPE can be emulsified to form particles of ~100–200 nm in diameter, allowing for cellular uptake via endocytosis (4). DCs are labeled with PFPE (PFPE-DCs) for ^19^F magnetic resonance imaging (MRI).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(PFPE + DCs)+AND+synthesis%0D%0A)]

Ahrens et al. briefly described the detailed preparation of PFPE-DCs (4). First, commercially available PFPE was emulsified (40% vol/vol) in a mixture of H_2_O, 2% lecithin, and 2% safflower oil to produce PFPE nanoparticles ~100–200 nm in diameter. Two types of DCs were used for labeling: a fetal skin-derived DC line (FSDCs) and primary cells derived from bone marrow (BMDCs). For FSDCs, the cells were labeled by incubating PFPE emulsion (2 μl/ml) with dendritic cells for 18 h at 37 ºC. The labeled cells (PFPE-FSDCs) were then suspended in solution. Adding transfection agents such as lipofectamine enhanced the labeling efficiency up to 26-fold with the same incubation time. For BMDCs, PFPE emulsion (2 μl/ml) was added to the bone marrow culture and incubated for 18 h at 37 ºC. The harvested PFPE-labeled BMDCs (PFPE-BMDCs) were then incubated on a poly-L-lysine–coated plate for 1 h at 37 ºC to adhere cells. Dead and non-adherent cells were discarded. The adherent cells were removed with trypsin-EDTA treatment to yield a BMDC purity of 80–90% as determined with flow cytometry for the expression of DC marker CD11c. The amount of PFPE was found to be 5.2 × 10^12^ fluorine spins (~0.25 ng PFPE) per FSDC or BMDC as determined with ^19^F NMR, allowing for detection of ~2×10^5^ labeled cells per voxel.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(PFPE + DCs)+AND+%22in+vitro%22)]

Ahrens et al. used ^19^F NMR to examine the intracellular retention of the PFPE in DCs in vitro (4). The ^19^F signal for PFPE-FSDCs was monitored with an 11.7-T (^19^F resonant frequency 470 MHz) NMR spectrometer for 5 d. The cell division caused dilution that led to a decrease in ^19^F signal; ~15% signal was observed after 5 d. During this time, the PFPE appeared to remain stable in that no change was found in its spectral line shape. The cellular internalization of PFPE emulsion particles was examined with fluorescence microscopy and transmission electron microscopy. FSDCs were fluorescence-labeled with fluorescein isothiocyanate-dextran (FITC-DX). The PFPE was also tagged with a fluorescent probe, lipophilic dialkycarbocyanine (DiI) fluorophore, in the presence of lipofectamine. Then the fluorescence-labeled FSDCs were incubated with the fluorescence-labeled PFPE for 18 h at 37 ºC as before. Under an electron microscope, the intracellular PFPE particles appeared as numerous, bright, smooth spheroids located within the macropinosomes, which are large vesicular compartments containing fluorescein. The osmium staining used to visualize intracellular structures also demonstrated the presence of unsaturated lipids in the particle's surfactant. Some PFPE particles were clustered together or wrapped with surrounded multiple membrane compartments relating to MHC class II–enriched compartments.

Ahrens et al. examined the effects of PFPE on cellular toxicity, proliferation, metabolism, and phenotype of labeled DCs were examined in vitro (4). The cytotoxicity of PFPE was evaluated with an assay that measured the leakage of the enzyme glucose 6-phosphate dehydrogenase (G6PD) from the cytoplasm into the culture medium. Little or no apparent cytotoxicity was found for all conditions studied. The cellular proliferation was assayed with methyl thiazole tetrazolium (MTT) and the total double-stranded DNA (dsDNA), which was further confirmed by direct cell counts. No apparent difference in cell proliferation was found between labeled cells and controls. The effect on cellular phenotype was examined via flow cytometric analysis of cellular markers. Several surface markers in the labeled DCs were compared with those in the unlabeled DCs, including the co-stimulatory molecule CD80 and MHC class II. The presence of PFPE emulsion particles or the transfection agent lipofectamine did not appear to induce maturation of DCs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(PFPE + DCs) +AND++rodentia)]

Ahrens et al. examined the migration of PFPE-DCs in mice with in vivo ^19^F MRI/^1^H MRI (4). Mice were injected with 8 × 10^6^ PFPE-FSDCs intramuscularly. T_2_-Weighted ^1^H images and ^19^F images were collected with an 11.7-T imager 8 h after the injection. The hyperintense sites in the ^1^H images, which reflected the presence of inflammatory cells or excess phosphates, appeared to correspond to sites with strong signals in ^19^F images. From these sites, the ^19^F signals were tracked farther away as a sign of DC migration to the draining lymph node. Ahrens et al. then studied the migration of PFPE-BMDCs from the foot to the lymph nodes (4). Mice received 4 × 10^6^ PFPE-BMDCs via subcutaneous injection into the tip of the hind footpad. ^19^F/^1^H images collected 6 h after injection exhibited a strong ^19^F signal (signal/noise ratio >10) in the popliteal lymph node located adjacent to the knee, which suggests that the cells migrate towards the lymph node. To confirm this migration pattern, the BMDCs were double-labeled with PFPE and 5-chloromethylfluorescein diacetate. Control mice were injected in one foot with the double-labeled BMDCs and in the other foot with PFPE-BMDCs. The efferent popliteal node and the inguinal/axillary nodes as controls were excised 24 h after injection. Single-cell suspensions were prepared from these excised tissues and analyzed with flow cytometry. Fluorescent cells were visible in the popliteal lymph nodes of mice receiving double-labeled BMDCs but not in mice that received PFPE-BMDCs. The biodistribution of PFPE-FSDCs was examined in mice with in vivo ^19^F MRI/^1^H MRI (4). Mice received an intravenous injection of 18 × 10^6^ PFPE-FSDCs, and ^19^F/^1^H images were collected after inoculation. A strong ^19^F signal (signal/noise ratio ~9) was found in the liver and spleen, and a weak signal was observed in the lung.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(PFPE + DCs) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(PFPE + DCs) +AND+human)]

No publication is currently available.

### NIH Support

EB003453, EB001977, ES012359

## References

1 Banchereau J., Steinman R.M. (1998). Dendritic cells and the control of immunity. Nature.
2 Pham W., Xie J., Gore J.C. (2007). Tracking the migration of dendritic cells by in vivo optical imaging. Neoplasia.
3 Banchereau J., Palucka A.K. (2005). Dendritic cells as therapeutic vaccines against cancer. Nat Rev Immunol.
4 Ahrens E.T., Flores R., Xu H., Morel P.A. (2005). In vivo imaging platform for tracking immunotherapeutic cells. Nat Biotechnol.
5 Bonasio R., von Andrian U.H. (2006). Generation, migration and function of circulating dendritic cells. Curr Opin Immunol.
6 Yu J.X., Kodibagkar V.D., Cui W., Mason R.P. (2005). 19F: a versatile reporter for non-invasive physiology and pharmacology using magnetic resonance. Curr Med Chem.
7 Zhang W., Ito Y., Berlin E., Roberts R., Berkowitz B.A. (2003). Role of hypoxia during normal retinal vessel development and in experimental retinopathy of prematurity. Invest Ophthalmol Vis Sci.
8 Noth U., Morrissey S.P., Deichmann R., Jung S., Adolf H., Haase A., Lutz J. (1997). Perfluoro-15-crown-5-ether labelled macrophages in adoptive transfer experimental allergic encephalomyelitis. Artif Cells Blood Substit Immobil Biotechnol.
9 Noth U., Rodrigues L.M., Robinson S.P., Jork A., Zimmermann U., Newell B., Griffiths J.R. (2004). In vivo determination of tumor oxygenation during growth and in response to carbogen breathing using 15C5-loaded alginate capsules as fluorine-19 magnetic resonance imaging oxygen sensors. Int J Radiat Oncol Biol Phys.